# ^99m^Tc-Ethylenedicysteine-endostatin

Chemical name: | ^99m^Tc-Ethylenedicysteine-endostatin
Abbreviated name: | ^99m^Tc-EC-endostatin
Synonym:
Agent category: | Polypeptide
Target: | Endostatin receptor
Target category: | Receptor
Method of detection: | Single photon emission computed tomography (SPECT)
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71981419), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_059957.3) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=80781) for more information about endostatin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-EC%5BAll%20Fields%5D%20AND%20endostatin)]

Angiogenesis is the formation of new blood capillaries and vessels from existing vessels (1-3). It involves the degradation of the basal membrane surrounding the parental vasculature, and the proliferation of endothelial and smooth muscle cells to form new vessels, resulting in an improvement in tissue perfusion and function. The major stimuli for angiogenesis include ischemia, hypoxia, inflammation, and shear stress (4). A large number of endogenous angiogenic factors are involved in angiogenesis (5), including vascular endothelial growth factor (VEGF), basic fibroblast growth factor (bFGF), interleukin-8 (IL-8), and transforming growth factor-β (TGF-β). Extracellular matrix and proteolytic enzymes as well as integrins are also involved during angiogenesis (6). There are also endogenous inhibitors of angiogenesis such as, angiostatin, endostatin and platelet factor-4 (7, 8).

Tumor angiogenesis represents a continuous and important process in tumor development in which the tumor attempts to gain an independent blood supply (9). This process is driven by the tumor's chronic overproduction of angiogenic factors, which bind to receptors on nearby vessel endothelial cells. Angiogenesis is essential for the growth of solid tumors and their metastases. Imaging angiogenesis may be useful for monitoring angiogenic treatments of tumors and cardiovascular diseases (3, 10, 11).

Endostatin was discovered as an endogenous inhibitor of tumor angiogenesis and endothelial-cell growth (12). It is one of the most promising anti-angiogenic cancer drugs. It has been successfully radiolabeled with ^99m^Tc for single photon emission computed tomography (SPECT) imaging of endostatin receptor density in tumors in rats (13). ^99m^Tc-EC-endostatin may prove to be a useful imaging tracer for selecting patients for anti-angiogenic treatment.

### Related Resource Links:

- Chapters in MICAD (Endostatin (http://www.ncbi.nlm.nih.gov/books?term=Endostatin%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Endostain (http://www.ncbi.nlm.nih.gov/gene/80781))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Endostatin (http://www.ncbi.nlm.nih.gov/omim/120328))
- Clinical trials (Endostatin (http://www.clinicaltrials.gov/ct2/results?term=endostatin))
- Drug information in FDA (Endostatin (http://google2.fda.gov/search?q=endostatin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=0&y=0))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-EC%5BAll%20Fields%5D%20AND%20endostatin%20and%20synthesis)]

L, L-Ethylenedicysteine (EC) was conjugated to amino or lysine residues of endostatin using sulfo-N-hydroxysulfosuccinimide. Ten EC (M_r_ 268) residues were estimated to conjugate to endostatin (M_r_ 20,000) to form EC-endostatin. ^99m^Tc was complexed to EC-endostatin to form ^99m^Tc-EC-endostatin with a radiochemical yield of 70-75% and a radiochemical purity of >97% (13). The specific activity was calculated to be 37 GBq/μmol (1.0 Ci/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-EC%5BAll%20Fields%5D%20AND%20endostatin%20and%20in%20vitro)]

Cell viability assays were performed using RBA CRL-1747 rat breast cancer cell line (13). EC-endostatin and endostatin showed similar cell death from 0.1 to 100 μM. Cellular uptake of 0.31 μM^99m^Tc-EC-endostatin was blocked (20-50%) by unlabeled endostatin (10-16 μM). Terminal deoxynucleotidyl transferase-mediated nick end labeling (TUNEL) assays showed that EC-endostatin and endostatin caused 19.87% and 19.43% cell apoptosis in human endothelial cells at 2 mg/ml, respectively. ^99m^Tc-EC-endostatin was stable in dog serum at 37ºC for 0.5-24 h as measured by thin-layer chromatography (TLC).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-EC%5BAll%20Fields%5D%20AND%20endostatin%20and%20rodentia)]

Rats were inoculated with RBA CRL-1747 tumor cells, followed by intravenous injection (0.37 MBq/rat, 10 μCi/rat, 10 μg/rat) of ^99m^Tc-EC-endostatin or ^99m^Tc-EC 14 -17 days after tumor transplantation (13). Tumor/tissue uptake ratios for ^99m^Tc-EC-endostatin rats increased as a function of time as compared with ^99m^Tc-EC. Tumor uptake in rats receiving ^99m^Tc-EC-endostatin was about 1-fold higher than rats receiving ^99m^Tc-EC. The liver and kidneys are the organs with high uptakes of both tracers. Both tracers were excreted mainly in the urine.

Scintigraphic images of rats given ^99m^Tc-EC-endostatin (11 MBq/rat, 300 μCi/rat, 300 μg/rat) showed that tumors could be well visualized at 0.5-4.0 h (13). Pretreatment of rats with molar excess of unlabeled endostatin blocked the uptake by 30-40%. Decreased tumor/non-tumor uptake of radiolabeled endostatin on day 7 after endostatin or paclitaxel treatment correlated to decreased tumor volume as well as decreased expression of VEGF, bFGF, and IL-8. Hence, the decrease in tumor uptake of ^99m^Tc-EC-endostatin was because of effective anti-tumor activity. The response of breast cancer cells grown in rats to the anti-angiogenic agents could be monitored non-invasively with ^99m^Tc-EC-endostatin.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-EC%5BAll%20Fields%5D%20AND%20endostatin%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-EC%5BAll%20Fields%5D%20AND%20endostatin%20and%20%28primates%20not%20humans%29)]

No publication is currently available

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-EC%5BAll%20Fields%5D%20AND%20endostatin%20and%20humans)]

No publication is currently available.

## NIH Support

CA16672

## References

1 Battegay E.J. (1995). Angiogenesis: mechanistic insights, neovascular diseases, and therapeutic prospects. J Mol Med.
2 Folkman J. (2003). Fundamental concepts of the angiogenic process. Curr Mol Med.
3 Sinusas A.J. (2004). Imaging of angiogenesis. J Nucl Cardiol.
4 Carmeliet P. (2003). Angiogenesis in health and disease. Nat Med.
5 Folkman J. (2003). Angiogenesis and proteins of the hemostatic system. J Thromb Haemost.
6 Carmeliet P. (2000). Mechanisms of angiogenesis and arteriogenesis. Nat Med.
7 Folkman J. (2004). Endogenous angiogenesis inhibitors. Apmis.
8 O'Reilly M.S., Holmgren L., Shing Y., Chen C., Rosenthal R.A., Cao Y., Moses M., Lane W.S., Sage E.H., Folkman J. (1994). Angiostatin: a circulating endothelial cell inhibitor that suppresses angiogenesis and tumor growth. Cold Spring Harb Symp Quant Biol.
9 Folkman J. (1995). Angiogenesis in cancer, vascular, rheumatoid and other disease. Nat Med.
10 Carmeliet P. (2004). Manipulating angiogenesis in medicine. J Intern Med.
11 Miller J.C., Pien H.H., Sahani D., Sorensen A.G., Thrall J.H. (2005). Imaging angiogenesis: applications and potential for drug development. J Natl Cancer Inst.
12 O'Reilly M.S., Boehm T., Shing Y., Fukai N., Vasios G., Lane W.S., Flynn E., Birkhead J.R., Olsen B.R., Folkman J. (1997). Endostatin: an endogenous inhibitor of angiogenesis and tumor growth. Cell.
13 Yang D.J., Kim K.D., Schechter N.R., Yu D.F., Wu P., Azhdarinia A., Roach J.S., Kalimi S.K., Ozaki K., Fogler W.E., Bryant J.L., Herbst R., Abbruzzes J., Kim E.E., Podoloff D.A. (2002). Assessment of antiangiogenic effect using 99mTc-EC-endostatin. Cancer Biother Radiopharm.